# Thiol-modified poly(ethylene glycol)-conjugated gold/superparamagnetic iron oxide nanoparticles

Chemical name: | Thiol-modified poly(ethylene glycol)-conjugated gold/superparamagnetic iron oxide nanoparticles
Abbreviated name: | PEG-S-Au/SPIO
Synonym: | PEG-S-Au/Feridex
Agent category: | Nanoparticle
Target: | Non-targeted
Target category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PEG%20Gold%20SPIO)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. SPIO nanoparticles are sometimes modified with dextran, poly(ethylene glycol) (PEG), or other biomaterials to reduce RES uptake and to prolong blood half-life. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific molecular imaging studies. SPIO agents are classified by their sizes with coating material (~20–3,500 nm in diameter) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and monocrystalline iron oxide nanoparticles (MION) (1).

Gold (Au) are easily added to SPIO nanoparticles with electron beam irradiation of a solution of Au and SPIO to form Au/SPIO (2). The Au moieties are highly reactive with the thiol group via a strong Au-S bond. Kojima et al. (3) coated the Au/SPIO nanoparticles with a thiol-modified PEG (PEG-S) to form PEG-S-Au/SPIO nanoparticles to study tumor accumulation in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=SPIO+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad) (SPIO)
- Clinical trials (Feridex (http://www.clinicaltrials.gov/ct2/results?term=Feridex))
- Drug information in FDA (Feridex (http://google2.fda.gov/search?q=Feridex&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=6))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PEG%20Gold%20SPIO%20and%20synthesis)]

A solution of SPIO nanoparticles (0.1 g/L), AuHCl_4_ (0.5 mM), 2-propanol (4.125 mM), and poly(vinyl alcohol) (10 mg/mL) was irradiated with an electron beam at a dose of 6 kGy (3). Au/SPIO nanoparticles were purified with high-speed centrifugation. AU/SPIO nanoparticles were mixed with thiol-modified PEG (PEG-S, 5 kDa) at a concentration of 1,000 mM PEG-S per 1 mg of Fe for 1 h at room temperature. The molar ratio of Fe/Au was determined to be 3.3. The amount of immobilized PEG-S was 1.74 mg PEG-S/mg Au. The hydrodynamic sizes of SPIO, Au/SPIO, and PEG-S-Au/SPIO were 69 nm, 164 nm, and 154 nm, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PEG%20Gold%20SPIO%20and%20in%20vitro)]

The Au-S bond of PEG-S-Au/SPIO remained intact in fetal bovine serum at 37°C after 60 min of incubation (3). Au/SPIO and PEG-S-Au/SPIO exhibited similar T2 relaxation times (1.5 T).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PEG%20Gold%20SPIO%20and%20rodentia)]

Kojima et al. (3) performed ex vivo biodistribution studies in mice (n = 3/group) bearing Meth-A tumors after injection of Au/SPIO and PEG-S-Au/SPIO (1 mg Fe). PEG-S-Au/SPIO had a significantly higher blood concentration (P < 0.001) than Au/SPIO at 2, 5, 10, 30, and 60 min after injection. PEG-S-Au/SPIO exhibited a Fe concentration ~40% lower than that of Au/SPIO in the liver at 1 h and 24 h after injection, whereas PEG-S-Au/SPIO showed a Fe concentration 10-fold higher than that of Au/SPIO in the tumor at the same time points. MRI imaging was performed at 1.5 T in mice bearing Meth-A tumors at 1 h after injection of SPIO, AU/SPIO, and PEG-S-Au/SPIO. T2-Weighted images showed that PEG-S-Au/SPIO decreased the signal intensity of the tumor with clear visualization of the tumor. On the other hand, SPIO and Au/SPIO did not improve the tumor contrast. Histological staining of Fe in the tumor tissue sections revealed that PEG-S-Au/SPIO leaked from the tumor blood vessels into the surrounding tumor tissue, whereas SPIO and Au/SPIO were not detected in the tumor tissue sections.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PEG%20Gold%20SPIO%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PEG%20Gold%20SPIO%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PEG%20Gold%20SPIO%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Mizukoshi Y., Seino S., Okitsu K., Kinoshita T., Otome Y., Nakagawa T., Yamamoto T.A. (2005). Sonochemical preparation of composite nanoparticles of Au/gamma-Fe2O3 and magnetic separation of glutathione. Ultrason Sonochem.
3 Kojima H., Mukai Y., Yoshikawa M., Kamei K., Yoshikawa T., Morita M., Inubushi T., Yamamoto T.A., Yoshioka Y., Okada N., Seino S., Nakagawa S. (2010). Simple PEG conjugation of SPIO via an Au-S bond improves its tumor targeting potency as a novel MR tumor imaging agent. Bioconjug Chem.